# Annexin A5-quantum dot-DTPA-gadolinium

Chemical name: | Annexin A5-quantum dot-DTPA-gadolinium
Abbreviated name: | AnxA5-QD-Gd
Synonym:
Agent Category: | Peptide
Target: | Phosphatidylserine
Target Category: | Binding
Method of detection: | Optical, near-infrared (NIR) and MRI
Source of signal/contrast: | Quantum dot, gadolinium
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=468888), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=4809273) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=308) for more information about annexin V.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Quantum%20dots%20and%20annexin)]

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when visible light (350-700 nm) absorbing fluorophores are used. Near-infrared (NIR) fluorescence (700-1000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging in small animals (4).

Fluorescent semiconductor quantum dots (QDs) are nanocrystals made of CdSe/CdTe-ZnS with radii of 1-10 nm (5-7). They can be tuned to emit in a range of wavelengths by changing their sizes and composition, thus providing broad excitation profiles and high absorption coefficients. They have narrow and symmetric emission spectra with long, excited-state lifetimes, 20-50 ns, as compared with 1-10 ns of fluorescent dyes. They process good quantum yields of 40-90% and high extinction coefficients. They are more photo-stable than conventional organic dyes. They can be coated and capped with hydrophilic materials for additional conjugations with biomolecules, such as peptides, antibodies, nucleic acids, and small organic compounds, which were tested in vitro and in vivo (7-11). Although many cells have been labeled with QDs in vitro with little cytotoxicity, there are only limited studies of long-term toxicity of QDs in small animals (12-20). However, little is known about the toxicity and the mechanisms of clearance and metabolism of QDs in humans.

Apoptosis (programmed cell death) plays an important role in the pathophysiology of many diseases, such as cancer, neurodegenerative disorders, vascular disorders, and chronic hepatitis, as well as in the biology of normal cells like epithelial cells and immune cells (21). During apoptosis, there is rapid redistribution of phosphatidylserine (PS) from the inner membrane leaflet to the outer membrane leaflet, exposing the anionic head group of PS. PS is also accessible for annexin V binding in necrosis because of disruption of the plasma membrane. Annexin V binds to PS with high affinity (K_d_ = 7 nM). Annexin V has been radiolabeled with ^123^I, ^124^I, and ^99m^Tc for single photon emission computed tomography (SPECT) imaging (22-24). Recently, annexin V was successfully labeled with ^18^F (25, 26). ^18^F-labeled annexin V is being developed as a positron emission tomography (PET) agent for imaging apoptosis as well as necrosis. Cy5.5-Annexin V and QD-annexin V (27) have been evaluated as optical probes for NIR imaging. Various bimodal annexin V-conjugated nanoparticles have been developed for imaging apoptosis, such as annexin V-CLIO-Cy5.5 (AnxCLIO-Cy5.5) and annexin V-QD-gadolinium (AnxA5-QD-Gd) for NIR and magnetic resonance (MR) imaging (28, 29). AnxA5-QD-Gd is being studied as a multimodality contrast agent for imaging apoptosis.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Quantum%20dots%20and%20annexin%20and%20synthesis)]

Core shell CdSe-ZnS QDs (with emission peaks at either 525 or 585 nm) coated with 8-12 streptavidin molecules were mixed with equimolar amount of biotinylated annexin V to form AnxA5-QDs (28). A minor excess of biotinylated Gd-DTPA or Gd-wedge (with eight Gd-DTPA complexes) was used to saturate the unoccupied biotin binding sites of streptavidin. This procedure yielded complexes with average stoichiometries of QD:AnxA5:Gd of 1:1:30 for AnxA5-QD-Gd and 1:1:240 for AnxA5-QD-wedge. The assembled QDs have a spherical diameter of 6.7 ± 1.0 nm, as measured by low-temperature transmission electron microscopy. AnxA5-QD-Gd and AnxA5-QD-Gd-wedge have r_1_ values per nanoparticle of 420-630 mM^-1^ s^-1^ and 3,000-4,500 mM^-1^ s^-1^, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Quantum%20dots%20and%20annexin%20and%20in%20vitro)]

Prinzen et al. (28) examined the property of AnxA5-QD-Gd and AnxA5-QD-Gd-wedge nanoparticles to discriminate between living and dying cells using two-photon laser scanning microscopy. Jurkat T cells were triggered to execute apoptosis by activation of Fas receptor using anti-Fas antibodies. Binding of AnxA5-QD-Gd and AnxA5-QD-Gd-wedge occurred to early and late apoptotic cells but not to viable cells. During early apoptosis, small patches of green fluorescence were visible on the cellular membrane, whereas during late apoptosis, the entire cellular membrane was brightly fluorescent. The late apoptotic phase was characterized by loss of plasma membrane integrity and fragmented nucleus. In addition, AnxA5-QD-Gd was able to be internalized by Jurkat T cells, as was reported for AnxA5. After incubation with AnxA5-QD-Gd, apoptotic Jurkat T cells exhibited a MRI signal intensity that was 5.9 and 6.9 folds higher as compared to buffer alone and Gd-wedge, respectively. Cells incubated with AnxA5-QD-Gd-wedge exhibited a MRI signal intensity that was 5.8 folds higher than AnxA5-QD-Gd, demonstrating that AnxA5-QD-Gd-wedge has a much better T1-lowering effect than AnxA5-QD-Gd, as was expected from the differences in r_1_. This resulted in a higher MRI signal intensity in T1-weighted imaging using the same amount of nanoparticles.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Quantum%20dots%20and%20annexin%20and%20rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Quantum%20dots%20and%20annexin%20and%20%28dog%20or%20sheep%20or%20pig%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Quantum%20dots%20and%20annexin%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Quantum%20dots%20and%20annexin%20and%20human)]

No publication is currently available.

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
3 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
4 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
5 Chan W.C., Maxwell D.J., Gao X., Bailey R.E., Han M., Nie S. (2002). Luminescent quantum dots for multiplexed biological detection and imaging. Curr Opin Biotechnol.
6 Gao X., Nie S. (2005). Quantum dot-encoded beads. Methods Mol Biol.
7 Michalet X., Pinaud F.F., Bentolila L.A., Tsay J.M., Doose S., Li J.J., Sundaresan G., Wu A.M., Gambhir S.S., Weiss S. (2005). Quantum dots for live cells, in vivo imaging, and diagnostics. Science.
8 Alivisatos A.P., Gu W., Larabell C. (2005). Quantum dots as cellular probes. Annu Rev Biomed Eng.
9 Hilger I., Leistner Y., Berndt A., Fritsche C., Haas K.M., Kosmehl H., Kaiser W.A. (2004). Near-infrared fluorescence imaging of HER-2 protein over-expression in tumour cells. Eur Radiol.
10 Medintz I.L., Uyeda H.T., Goldman E.R., Mattoussi H. (2005). Quantum dot bioconjugates for imaging, labelling and sensing. Nat Mater.
11 Smith A.M., Gao X., Nie S. (2004). Quantum dot nanocrystals for in vivo molecular and cellular imaging. Photochem Photobiol.
12 Akerman M.E., Chan W.C., Laakkonen P., Bhatia S.N., Ruoslahti E. (2002). Nanocrystal targeting in vivo. Proc Natl Acad Sci U S A.
13 Braydich-Stolle L., Hussain S., Schlager J.J., Hofmann M.C. (2005). In vitro cytotoxicity of nanoparticles in mammalian germline stem cells. Toxicol Sci.
14 Frangioni J.V., Hajjar R.J. (2004). In vivo tracking of stem cells for clinical trials in cardiovascular disease. Circulation.
15 Gao X., Cui Y., Levenson R.M., Chung L.W., Nie S. (2004). In vivo cancer targeting and imaging with semiconductor quantum dots. Nat Biotechnol.
16 Han M., Gao X., Su J.Z., Nie S. (2001). Quantum-dot-tagged microbeads for multiplexed optical coding of biomolecules. Nat Biotechnol.
17 Lovric J., Bazzi H.S., Cuie Y., Fortin G.R., Winnik F.M., Maysinger D. (2005). Differences in subcellular distribution and toxicity of green and red emitting CdTe quantum dots. J Mol Med.
18 Ohnishi S., Lomnes S.J., Laurence R.G., Gogbashian A., Mariani G., Frangioni J.V. (2005). Organic alternatives to quantum dots for intraoperative near-infrared fluorescent sentinel lymph node mapping. Mol Imaging.
19 Shiohara A., Hoshino A., Hanaki K., Suzuki K., Yamamoto K. (2004). On the cyto-toxicity caused by quantum dots. Microbiol Immunol.
20 Soltesz E.G., Kim S., Laurence R.G., DeGrand A.M., Parungo C.P., Dor D.M., Cohn L.H., Bawendi M.G., Frangioni J.V., Mihaljevic T. (2005). Intraoperative sentinel lymph node mapping of the lung using near-infrared fluorescent quantum dots. Ann Thorac Surg.
21 Thompson C.B. (1995). Apoptosis in the pathogenesis and treatment of disease. Science.
22 Blankenberg F.G. (2004). Recent advances in the imaging of programmed cell death. Curr Pharm Des.
23 Lahorte C., Slegers G., Philippe J., Van de Wiele C., Dierckx R.A. (2001). Synthesis and in vitro evaluation of 123I-labelled human recombinant annexin V. Biomol Eng.
24 Keen H.G., Dekker B.A., Disley L., Hastings D., Lyons S., Reader A.J., Ottewell P., Watson A., Zweit J. (2005). Imaging apoptosis in vivo using 124I-annexin V and PET. Nucl Med Biol.
25 Toretsky J., Levenson A., Weinberg I.N., Tait J.F., Uren A., Mease R.C. (2004). Preparation of F-18 labeled annexin V: a potential PET radiopharmaceutical for imaging cell death. Nucl Med Biol.
26 Zijlstra S., Gunawan J., Burchert W. (2003). Synthesis and evaluation of a 18F-labelled recombinant annexin-V derivative, for identification and quantification of apoptotic cells with PET. Appl Radiat Isot.
27 Schellenberger E.A., Sosnovik D., Weissleder R., Josephson L. (2004). Magneto/optical annexin V, a multimodal protein. Bioconjug Chem.
28 Prinzen L., Miserus R.J., Dirksen A., Hackeng T.M., Deckers N., Bitsch N.J., Megens R.T., Douma K., Heemskerk J.W., Kooi M.E., Frederik P.M., Slaaf D.W., van Zandvoort M.A., Reutelingsperger C.P. (2007). Optical and magnetic resonance imaging of cell death and platelet activation using annexin a5-functionalized quantum dots. Nano Lett.
29 van Tilborg G.A., Mulder W.J., Chin P.T., Storm G., Reutelingsperger C.P., Nicolay K., Strijkers G.J. (2006). Annexin A5-conjugated quantum dots with a paramagnetic lipidic coating for the multimodal detection of apoptotic cells. Bioconjug Chem.